# ^111^In-TA138

Chemical name: | ^111^In-TA138
Abbreviated name: | RP748
Synonym:
Agent category: | Compound
Target: | α_v_β_3_ integrin
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal/contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D)]

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). They consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). The α_v_β_3_ integrin is strongly expressed on tumor cells, activated endothelial cells (3), and arterial smooth muscle cells (8). In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (4, 9, 10), and the agonists are being studied as angiogenic agents for coronary angiogenesis (11, 12). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) was identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_. Various radiolabeled antagonists and peptides were introduced for imaging of tumors and tumor angiogenesis (13).

TA138, an antagonist to the α_v_β_3_ integrin, was developed based on SH066 (a quinolone-based vitronectin receptor antagonist) (14). TA138 contains a DOTA moiety for ^111^In labeling. ^111^In-TA138 (RP748) was found to have a high accumulation in a spontaneous mammary adenocarcinoma (α_v_β_3_-positive) in the c-Neu Oncomouse model (14, 15). The binding of ^111^In-TA138 to the integrin receptor was found to be specific both in vitro and in vivo.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D%29%20AND%20synthesis%5BAll%20Fields%5D)]

A detailed chemical synthesis of TA138 (3-sulfon-N-[[4,7,10-tris(carboxymethyl)1,4,7,10-tetraazacyclododec-1-yl]acetyl]-L-alanyl-N-[2-[4-[[[(1S)-1-carboxy-2[[[1,4-dihydro-7-[(1H-imidazol-2-ylamino]methyl]-1-methyl-4-oxo-3-quinolinyl]carbonyl]amino]ethyl]amino]-sulfonyl]-3,5-dimethylphenoxy]-1-oxobutyl]amino]ethyl]-3-sulfo-L-alaninamide) was reported by Liu et al. (16). ^111^InCl_3_ solution (81.4 MBq, 2.2 mCi) was added to a solution of TA138 (100 μg) in ammonium acetate buffer (17). The mixture was heated at 100ºC for 5 min. The radiochemical purity of ^111^In-TA138 was 98% as measured by high-performance liquid chromatography (HPLC). The specific activity was 0.83 MBq/μg (22.5 μCi/μg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D%29%20AND%20in%20vitro)]

TA138 and SH066 were shown to inhibit α_v_β_3_-mediated binding of β3-transfected 293 human embryonic kidney cells with an IC_50_ of 12 ± 3 and 11 ± 3 nM, respectively (17). Neither compound inhibited α_IIb_β_3_, α_v_β_5,_ and α_5_β_1_ integrin in cell-based binding assays. TA138 and RP748 were reported to be effective in inhibiting α_v_β_3_-mediated adhesion of human endothelial cells to fibrinogen with an IC_50_ of 40 ± 1 and 42 ± 1 nM, respectively (18). In a chick chorioallantoic membrane model, TA138 (2 μg/ml) inhibited basic fibroblast growth factor-induced neovascularization by 50%. Activation of endothelial cells in culture by Mn^2+^ led to a 17-fold increase in ^111^In-TA138 binding affinity (K_d_) for α_v_β_3_ integrin from 374 nM to 21 nM and a 0.8-fold (B_max_) increase in binding sites/cell from 130,000 sites/cell to 230,000 sites/cell (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D%29%20AND%20rodentia)]

Biodistribution studies of ^111^In-TA138 were evaluated in the c-Neu Oncomouse spontaneous mammary tumor model (17). Whole-body small animal images by dynamic scintigraphy were obtained at 0.5, 1, and 2 h after injection of ^111^In-TA138 (74 MBq/kg, 2 mCi/kg). The tumor uptake of ^111^In-TA138 was visible at all time points. Tissue distribution of the tracer was studied at 2 and 24 h. ^111^In-TA138 showed high uptake of 9.4% injected dose (ID)/g in the tumor at 2 h and decreased to 3.5% ID/g at 24 h. ^111^In-TA138 was cleared rapidly from the blood with an initial half-life of 1.1 h. The non-targeted organ with the highest uptake was the uterus (4.71% ID/g), followed by the colon (3.84%), lung (2.74%), kidney (2.33%), stomach (2.23%), and liver (1.94%) at 2 h after injection. Very high radioactivity was found in the urine, indicating high renal excretion. There was a dose-dependent decrease in ^111^In-TA138 tumor uptake with increasing doses of TA138 (300-2100 μg/m^2^). Tumor accumulation was 8.3% ID/g and 1.8% ID/g when the TA138 dose was 0 and 2100 μg/m^2^, respectively. In a separate study, ^90^Y-TA138 uptake in the tumor and other organs was similar to ^111^In-TA138 in the c-Neu Oncomouse model (15). Therefore, ^90^Y-TA138 can be developed as a radiopharmaceutical for tumor treatment, and ^111^In-TA138 can be developed as an imaging agent for tumor detection.

^111^In-TA138 was able to detect vascular remodeling in apolipoprotein E-negative (apoE−^/^−) mice with left common carotid artery injury (11). There was a significantly higher uptake of ^111^In-TA138 in the injured artery than in the contralateral uninjured artery. A 50-fold excess of unlabeled TA138 decreased ^111^In-TA138 uptake by 72%, demonstrating specificity of accumulation of radioactivity. Immunohistochemical studies confirmed an increase in expression of α_v_β_3_ integrin in the injured arteries. There was also an increase in proliferation of vascular cells in the injured arteries.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D%29%20AND%20%28dog%20or%20rabbit%20or%20pig%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D%29%20AND%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=TA138%5BAll%20Fields%5D%20OR%20RP748%5BAll%20Fields%5D%29%20AND%20human)]

No publication is currently available.

## References

1 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
2 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
5 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
6 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
7 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
8 Moiseeva E.P. (2001). Adhesion receptors of vascular smooth muscle cells and their functions. Cardiovasc Res.
9 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
10 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
11 Sadeghi M.M., Krassilnikova S., Zhang J., Gharaei A.A., Fassaei H.R., Esmailzadeh L., Kooshkabadi A., Edwards S., Yalamanchili P., Harris T.D., Sinusas A.J., Zaret B.L., Bender J.R. (2004). Detection of injury-induced vascular remodeling by targeting activated alphavbeta3 integrin in vivo. Circulation.
12 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
13 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
14 Batt D.G., Petraitis J.J., Houghton G.C., Modi D.P., Cain G.A., Corjay M.H., Mousa S.A., Bouchard P.J., Forsythe M.S., Harlow P.P., Barbera F.A., Spitz S.M., Wexler R.R., Jadhav P.K. (2000). Disubstituted indazoles as potent antagonists of the integrin alpha(v)beta(3). J Med Chem.
15 Onthank D.C., Liu S., Silva P.J., Barrett J.A., Harris T.D., Robinson S.P., Edwards D.S. (2004). 90Y and 111In complexes of a DOTA-conjugated integrin alpha v beta 3 receptor antagonist: different but biologically equivalent. Bioconjug Chem.
16 Liu S., Harris T.D., Ellars C.E., Edwards D.S. (2003). Anaerobic 90Y- and 177Lu-labeling of a DOTA-conjugated nonpeptide vitronectin receptor antagonist. Bioconjug Chem.
17 Harris T.D., Kalogeropoulos S., Nguyen T., Liu S., Bartis J., Ellars C., Edwards S., Onthank D., Silva P., Yalamanchili P., Robinson S., Lazewatsky J., Barrett J., Bozarth J. (2003). Design, synthesis, and evaluation of radiolabeled integrin alpha v beta 3 receptor antagonists for tumor imaging and radiotherapy. Cancer Biother Radiopharm.
18 Mousa S.A., Mohamed S., Wexler E.J., Kerr J.S. (2005). Antiangiogenesis and anticancer efficacy of TA138, a novel alphavbeta3 antagonist. Anticancer Res.